# Cy5.5-Labeled and gadolinium-chelated chitosan nanoparticles

Chemical name: | Cy5.5-Labeled and gadolinium-chelated chitosan nanoparticles
Abbreviated name: | Cy5.5-CNP-Gd(III)
Synonym:
Agent Category: | Nanoparticles
Target: | Non-targeted
Target Category: | Non-targeted
Method of detection: | Multimodality imaging (optical/magnetic resonance imaging (OI/MRI))
Source of signal / contrast: | Cy5.5 and Gd(III)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=multimodality+imaging+and+review)]

The Cy5.5-labeled and gadolinium (Gd(III))-chelated chitosan nanoparticles, abbreviated as Cy5.5-CNP-Gd(III), are an optical/magnetic resonance (MR) dual imaging agent synthesized by Nam et al. for multimodality imaging of tumors (1).

The idea of using multiple modalities in a single imaging session comes from the fact that modalities with high sensitivity have relatively poor resolution, while those with high resolution have relatively poor sensitivity (2, 3). Integration of multiple modalities in imaging would take the advantages of each modality and allow better characterization of diseases and disease processes (4, 5). To date, the most successful hybrid system is derived from the fusion of positron emission tomography (PET) and computed tomography (CT) (5-8). PET is highly sensitive and allows three-dimensional images that show the concentration and location of the radiolabeled tracers of interest, while CT provides high-resolution imaging of the anatomical structures. Because of limited soft-tissue contrast and high X-ray radiation that accompanies CT imaging, considerable effort has been invested in recent years toward development of PET/magnetic resonance imaging (MRI) hybrid systems in an attempt to generate combined functional and morphological images with excellent soft tissue contrast, good spatial resolution of the anatomy, and accurate temporal and spatial image fusion (9-11). In contrast, systems integrated with optical techniques have not been investigated as extensively. Considering the advantages of multichannel imaging with single or multiple probes and the low cost of studying reporter gene expression in animal models, optical imaging integrated with other modalities may provide information at the cellular and molecular levels, which is critical in preclinical studies (1, 2, 12).

Development of hybrid imaging technology has triggered great effort in probe development to boost the benefits of hybrid instrument technology (12-15). In the case of optical/MRI probe design, the challenge is turned around to incorporate enough paramagnetic ions for detection by the relatively low sensitivity of MRI. Nam et al. have developed a dual imaging probe (Cy5.5-CNP-Gd(III)) with water-soluble glycol chitosan and the probes were preferably accumulated within the tumor xenografts in vivo (1). Chitosan has been frequently used to make nanoparticles carrying imaging reporters as well as therapeutic agents (1, 12, 15). Generally, the positively charged chitosan polymer can coat around a nanoparticle core by electrostatic adsorption, and other components are embedded in the chitosan matrix during the coating process. All components can also be entrapped simultaneously in the chitosan matrix.

### Related Resource Links:

- Multimodality imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=multimodality%5bAll+Fields%5d+OR+multimodal%5bAll+Fields%5d+AND+micad%5bbook%5d)
- Multimodality imaging clinical trials in ClinicalTrial.gov (http://clinicaltrials.gov/ct2/results?term=multimodality+imaging)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20201550)]

Nam et al. synthesized Cy5.5-CNP-Gd(III) by conjugating Cy5.5 to amphiphilic glycol chitosan (GC)-5β-cholanic acid (CA) conjugates (Cy5.5-GC-CA) and chelating Gd(III) with 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA)-modified Cy5.5-GC-CA conjugates (1). Briefly, biocompatible and water-soluble GC (50 kDa) was first chemically modified with CA to form an amide linkage between the amine group of GC and the carboxyl acid of CA, resulting in the GC-CA conjugate. The molecular weight of GC-CA was 54 kDa with 11 ± 2 CA molecules per GC. For optical imaging, 0.5 ± 0.1 dyes of Cy5.5 monohydroxysuccinimide ester were then conjugated to the GC-CA (Cy5.5-GC-CA). For MRI, DOTA was first directly conjugated to the amine groups in the Cy5.5-GC-CA, and Gd(III) was then chelated. The degree of substitution of the number of DOTA molecules per nanoparticle was in the range from 13 to 45. The weight ratio of Gd(III) was maximized to ~6 ± 0.28%. The Cy5.5-CNP-Gd(III) nanoparticles were spherical in shape and ~350 nm in diameter. In phosphate-buffered saline at 37°C, Cy5.5-CNP-Gd(III) nanoparticles remained dispersed and maintained their original size for up to 40 days. Strong fluorescent signals and identical T1-weighted images were obtained under different pH conditions (pH 5.2 and 7.4). These results indicate that the chelated Gd(III) ions are highly stable in the nanoparticles.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20201550)]

The cellular uptake and cytotoxicity of Cy5.5-CNP-Gd(III) were evaluated in vitro with HeLa H2B-GFP cells (1). After incubation of the cells with Cy5.5-CNP-Gd(III) for 1 h, Cy5.5-CNP-Gd(III) nanoparticles were rapidly taken up by the HeLa cells and were found in the cytoplasm of cells. Cy5.5-CNP-Gd(III) exhibited almost 100% cell viability even at relatively high concentrations up to 250 μg/ml after incubation for 24 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20201550)]

Biodistribution of Cy5.5-CNP-Gd(III) was analyzed with optical imaging after intravenous injection into nude mice bearing subcutaneous tumors of murine squamous carcinoma cells (SCC7) (1). Mice treated with Cy5.5-CNP-Gd(III) (n = 3 mice; 5 mg/kg) showed a strong near-infrared fluorescence (NIRF) signal throughout the whole body within 6 h after injection. Tumors were able to be delineated from the surrounding tissue from 6 h, exhibited the maximum NIRF signal from 12 h to 3 days, and were still visible for up to 5 days after injection. Ex vivo images of the excised tissues 1 day after injection showed that Cy5.5-CNP-Gd(III) was mainly taken up by the tumors and was not significantly taken up by normal tissues. The total photon counts per gram of each organ were three- to seven-fold higher in tumors than in other organs (liver, lungs, kidneys, heart, and tumors). Approximately 50% of the nanoparticles circulated for 23 h, indicating a prolonged blood lifetime.

Optical/MR dual imaging was also performed in the SCC7 tumor-bearing mice (1). Both NIRF optical and MRI (1.5 T) readily detected the tumors at 1 day after injection of Cy5.5-CNP-Gd(III) (5 mg/kg). With T1-weighted imaging, the margin of the tumor tissue could be clearly delineated, indicating efficient nanoparticle accumulation at the tumor site. After 1 day, the relative signal enhancement (%) of tumors strongly increased from 70 to 162, compared with that of muscles (65 to 95), indicating that the nanoparticles had greater tumor targeting ability.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Nam T., Park S., Lee S.Y., Park K., Choi K., Song I.C., Han M.H., Leary J.J., Yuk S.A., Kwon I.C., Kim K., Jeong S.Y. (2010). Tumor targeting chitosan nanoparticles for dual-modality optical/MR cancer imaging. Bioconjug Chem.
2 Cherry S.R. (2006). Multimodality in vivo imaging systems: twice the power or double the trouble?. Annu Rev Biomed Eng.
3 Delbeke D., Schoder H., Martin W.H., Wahl R.L. (2009). Hybrid imaging (SPECT/CT and PET/CT): improving therapeutic decisions. Semin Nucl Med.
4 Cherry S.R. (2009). Multimodality imaging: beyond PET/CT and SPECT/CT. Semin Nucl Med.
5 Patel C.N., Goldstone A.R., Chowdhury F.U., Scarsbrook A.F. (2010). FDG PET/CT in oncology: "raising the bar. Clin Radiol.
6 Boss A., Bisdas S., Kolb A., Hofmann M., Ernemann U., Claussen C.D., Pfannenberg C., Pichler B.J., Reimold M., Stegger L. (2010). Hybrid PET/MRI of intracranial masses: initial experiences and comparison to PET/CT. J Nucl Med.
7 Chowdhury F.U., Shah N., Scarsbrook A.F., Bradley K.M. (2010). [18F]FDG PET/CT imaging of colorectal cancer: a pictorial review. Postgrad Med J.
8 Ell P.J. (2006). The contribution of PET/CT to improved patient management. Br J Radiol.
9 Pichler B.J., Kolb A., Nagele T., Schlemmer H.P. (2010). PET/MRI: paving the way for the next generation of clinical multimodality imaging applications. J Nucl Med.
10 Sauter, A.W., H.F. Wehrl, A. Kolb, M.S. Judenhofer, and B.J. Pichler, Combined PET/MRI: one step further in multimodality imaging. Trends Mol Med, 2010
11 Wehrl H.F., Judenhofer M.S., Wiehr S., Pichler B.J. (2009). Pre-clinical PET/MR: technological advances and new perspectives in biomedical research. Eur J Nucl Med Mol Imaging.
12 Louie A. (2010). Multimodality imaging probes: design and challenges. Chem Rev.
13 Jennings L.E., Long N.J. (2009). 'Two is better than one'--probes for dual-modality molecular imaging. Chem Commun (Camb).
14 Lee S., Chen X. (2009). Dual-modality probes for in vivo molecular imaging. Mol Imaging.
15 Majumdar D., Peng X.H., Shin D.M. (2010). The medicinal chemistry of theragnostics, multimodality imaging and applications of nanotechnology in cancer. Curr Top Med Chem.